# 3-Carboxy-2,2,5,5-tetramethyl-pyrrolidinyl-N-oxyl

Chemical name: | 3-Carboxy-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxyl
Abbreviated name: | 3CxP
Synonym: | 3-Carboxy-PROXYL, 3-carboxy-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxy, 3-carboxy-2,2,5,5-tetramethyl-1-pyrrolidin-1-yl--N-oxy free radical, PCA, 3-CTPY
Agent category: | Small molecule
Target: | Other
Target category: | Other-reactive oxygen species (ROS)
Method of detection: | Electron paramagnetic resonance imaging (EPRI), magnetic resonance imaging (MRI), proton electron double resonance imaging (PEDRI), Overhauser-enhanced MRI (OMRI)
Source of signal/contrast: | Nitroxide radicals
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=3-Carboxy-PROXYL)]

Reactive oxygen species (ROS) are various free radicals generated in a biological milieu (1, 2). They are propagated through a cascade of reactions in the pathogenesis in many diseases, including cancer, stroke, atherosclerosis, ischemia-reperfusion injury, Alzheimer’s disease, diabetic vascular diseases, and inflammatory diseases (2). In particular, ROS interact with glutathione (GSH), NADPH, and ascorbates to maintain cellular redox status (3). Therefore, the distribution of ROS in tissue can be used as a surrogate marker to characterize the redox status/environment in disease-related physiological and pathological conditions (1). Because all free radicals contain unpaired electrons, the electron paramagnetic resonance (EPR) technique, also called electron spin resonance (ESR,) is specific for detecting and quantifying ROS (2). EPR spectra can provide a wealth of information for unequivocal identification of free radicals, such as fine, hyperfine, and superhyperfine structures, g-factor, and lineshape (2). EPR imaging (EPRI) technique allows for non-invasive mapping of free radicals in animals/organs (4).

EPR is fundamentally similar to nuclear magnetic resonance (NMR) (5). However, the differences in the physical and chemical properties of the resonance species (unpaired electrons versus nuclear spin) lead to three major differences in acquiring the spectra/images: gyromagnetic ratio, relaxation time, and concentration (5). The gyromagnetic ratio of an electron spin is 658 times larger than that of a proton nuclear spin, resulting in a 658-fold increase in its magnetic moment and resonant frequency. For instance, with a magnet of 0.34 T, the EPR frequency of X-band is 9.5 GHz, and the NMR frequency of proton nuclei is 14.4 MHz. As a result of strong non-resonant water absorption, a high radiofrequency such as 9.5 GHz is not suitable for examining tissue samples. Thus, much lower EPR frequencies in the range of 1.2 GHz (L-band) to 300 MHz are used instead, corresponding to a penetration depth of a few cm. The increase in the magnetic moment of electron spin provides ~700 times greater intrinsic sensitivity with EPR on a molar basis than with NMR. Because the excited electron spins relax on a nanosecond time scale, which is several orders of magnitude shorter than the nuclear spin (measured in ms), pulsed EPR (Fourier transformation EPR (FT EPR) or time-domain EPR) is only applicable to those free radicals with an extremely narrow line, whereas most ERP spectrometers use the continuous wave technique (CW EPR). The lack of high concentrations of naturally occurring paramagnetic species such as free radicals often requires the addition of paramagnetic species. This in turn allows for the quantification of exogenous paramagnetic species but also requires the acquisition of anatomic information with different imaging modalities such as magnetic resonance imaging (MRI). Proton electron double resonance imaging (PEDRI), also called Overhauser-enhanced magnetic resonance imaging (OMRI)) is a double resonance technique that encodes characteristic EPR spectral information on a high-resolution MRI (6). This method uses EPR irradiation to saturate paramagnetic species and leads to polarization of water protons through the dynamic nuclear polarization (DNP) effect. The polarized protons produce enhanced signal intensity in MRI. PEDRI offers good sensitivity, high spatial resolution, and signal enhancement of approximately two orders of magnitude (7).

Nitroxides are stable organic free radicals that have a single unpaired electron delocalized between the nitrogen and the oxygen (8). The steric hindrance around the nitroxide group makes these compounds very stable. They can be obtained in pure form, and they can be stored and handled in the laboratory with no more precautions than most organic substances (9). Nitroxides used as the contrast agent in EPRI can detect the redox status on the basis of their reduction to EPR-silent hydroxylamine (10), and nitroxides have been extensively used in cells, tissues, and living animals (11). Inside cells, nitroxides are reduced to hydroxylamine by cellular antioxidants such as ascorbate, thioredoxin, reductase, ubiquinol, NADPH and GSH. Nitroxides also can function as superoxide dismutase mimics and repair DNA damage caused by ultraviolet irradiation. In addition to the use as an EPRI contrast agent, nitroxides are T_1_ relaxation agents in MRI for having an unpaired electron (12). Because their reduced form, hydroxylamine, is diamagnetic, the reduction process is accompanied by a decrease in T_1_ relaxivity. This decrease reflects the alterations in the redox status and can be used to map the redox status. Although the T_1_ relaxivity of nitroxides is much lower than that of gadolinium chelates (one unpaired electron versus seven unpaired electrons), their high cellular permeability leads to a significantly greater volume distribution in tissues and compensates for their lower relaxivity (12). Various nitroxides are designed to target different cellular compartments (8). For example, a neutral nitroxide can be distributed throughout the intracellular and extracellular environments, whereas a charged nitroxide is unable to cross the plasma membrane and can be used to measure oxygen levels in extracellular compartments. 3-Carboxy-2,2,5,5-tetramethyl-1-pyrrolidinyl-N-oxyl (3CxP) is a charged nitroxide that is available commercially. This nitroxide is unable to permeate the cell and exhibits minimal lipophilicity. As a piperidine nitroxide with a line width of 1.4 Gauss and low toxicity, 3CxP is suitable for EPRI and Overhauser-enhanced magnetic resonance imaging in intact animals (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carboxy-PROXYL)+AND+synthesis%0D%0A)]

3CxP was synthesized in several steps (13). First, acetone was condensed with ammonia in the presence of calcium chloride. The produced 4-oxo-2,2,6,6-tetramethylpiperidine (triacetoneamine) was converted to the corresponding nitroxyl radical (4-oxo-2,2,6,6-tetramethylpiperidinoxyl) by reaction with 30% hydrogen peroxide (14). The obtained nitroxyl radicals were then reacted with iodine in an alkaline medium to produce 2,2,5,5-tetramethylpyrrolinoxyl, which was hydrolyzed into 3CxP by hydrolysis (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( 3-Carboxy-PROXYL)+AND+%22in+vitro%22)]

The T_1_ relaxivity of 3CxP was determined to be ~0.2 mM^-1^s^-1^ (12). The partition coefficient of 3CxP in n-octanol/water was found to be 0.0047 (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carboxy-PROXYL) +AND++rodentia)]

Sano et al. reported the biodistribution of 3CxP in mice (4–5 weeks old, 17–23 g) (15). After intravenous injection of 100 μl of 150 mM 3CxP solution, blood was collected 3 min later and tissues were rapidly harvested and homogenized, including brain, liver, kidney, heart, lung, spleen, stomach, and muscle. Blood or homogenates were transferred into capillary tubes and observed with an X-band EPR spectrometer (9.4 GHz). The distribution of 3CxP in tissue (μmol spin/gram of tissue) was found to be 0.0 ± 0.0 in brain, 1.18 ± 0.06 in blood, 0.08 ± 0.02 in liver, 0.51 ± 0.21 in kidney, 0.28 ± 0.13 in heart, 0.39 ± 0.07 in lung, 0.27 ± 0.05 in spleen, 0.12 ± 0.03 in stomach, and 0.12 ± 0.06 in muscle. The distribution of 3CxP plus its reduced form (hydroxylamine) in tissue (μmol spin/gram of tissue) was found to be 0.02 ± 0.0 in brain, 1.27 ± 0.08 in blood, 1.15 ± 0.28 in liver, 1.65 ± 0.27 in kidney, 0.72 ± 0.04 in heart, 0.42 ± 0.07 in lung, 0.47 ± 0.04 in spleen, 0.16 ± 0.02 in stomach, and 0.18 ± 0.06 in muscle. Sano et al. also examined the in vivo distribution of 3CxP in mouse brain (15). After intravenous injection, two-dimensional images were collected with an L-band ESR-computed tomography system; in these images the signal of 3CxP appeared only in the extracranial domain. Okajo et al. measured the pharmacokinetics 3CxP in rats (8 weeks old) (16). After intravenous injection of 3CxP at a dose of 0.3 mmol/kg, pharmacokinetics were obtained with a blood circulation monitoring method using an X-band EPR spectrometer (9.4 GHz). The EPR signal decay in blood exhibited a biphasic profile with α-phase rate constant k_1_ of 0.444 ± 0.064 min^-1^ and β-phase rate constant k_2_ of 0.094 ± 0.0121 min^-1^.

Hyodo et al. used MRI to study the in vivo pharmacokinetics of 3CxP in tumors (12). C3H mice (6–8 weeks old, 20–30 g) were implanted with squamous cell carcinoma (SCCVII) in the right hind leg. After intravenous injection of 3CxP at a dose of 1 mmol/kg (150 mM), T_1_-weighted images were collected on a 4.7-T MRI imager. Maximum MRI intensity in the tumor area appeared at 9.3 min after injection, whereas the kidney exhibited continuous enhancements up to 17.8 min. There was no significant difference in the decay rate between the tumor (0.020 ± 0.014 min^-1^) and the normal leg (0.029 ± 0.014 min^-1^). The blood and organs were collected at 2.5, 7.5, 10, 15, and 20 min after injection, and the concentration of 3CxP in tissues was assessed with the use of an X-band EPR spectrometer. The levels of nitroxide plus nitroxylamine as a function of time did not demonstrate significant change during the imaging time in either tumor or muscle. Li et al. examined the distribution of 3CxP in mice (35 g) by PEDRI (11). After intravenously injecting 0.5 ml of 100 mM 3CxP solution, PEDRI was performed on a 0.38-T MRI imager (856 kHz NMR resonant frequency and 567 MHz EPR resonant frequency). 3CxP was found to distribute initially in the heart, lungs, major vessels, and kidneys. The image intensity peaked at ~2.5 min in the heart, lungs, and major vessels and at 5–10 min in the kidney, but returned to the preinjection levels at 30 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carboxy-PROXYL) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(3-Carboxy-PROXYL) +AND+human)]

No publication is currently available.

### NIH Support

EB004900, EB00890, EB00306, EB00254

## References

1 Soule B.P., Hyodo F., Matsumoto K., Simone N.L., Cook J.A., Krishna M.C., Mitchell J.B. (2007). Therapeutic and clinical applications of nitroxide compounds. Antioxid Redox Signal.
2 Kuppusamy P., Zweier J.L. (2004). Cardiac applications of EPR imaging. NMR Biomed.
3 Hirayama A., Nagase S. (2006). Electron paramagnetic resonance imaging of oxidative stress in renal disease. Nephron Clin Pract.
4 Mikuni T., He G., Petryakov S., Fallouh M.M., Deng Y., Ishihara R., Kuppusamy P., Tatsuta M., Zweier J.L. (2004). In vivo detection of gastric cancer in rats by electron paramagnetic resonance imaging. Cancer Res.
5 Gallez B., Swartz H.M. (2004). In vivo EPR: when, how and why?. NMR Biomed.
6 Matsumoto K., Narazaki M., Ikehira H., Anzai K., Ikota N. (2007). Comparisons of EPR imaging and T1-weighted MRI for efficient imaging of nitroxyl contrast agents. J Magn Reson.
7 Hyodo F., Murugesan R., Matsumoto K., Hyodo E., Subramanian S., Mitchell J.B., Krishna M.C. (2008). Monitoring redox-sensitive paramagnetic contrast agent by EPRI, OMRI and MRI. J Magn Reson.
8 Gallez B., Baudelet C., Jordan B.F. (2004). Assessment of tumor oxygenation by electron paramagnetic resonance: principles and applications. NMR Biomed.
9 Holtzman, J.L., ed. Spin labeling in pharmacology1984, Academic Press, INC: New York. 5.
10 Kroll C., Borchert H.H. (1999). Metabolism of the stable nitroxyl radical 4-oxo-2,2,6, 6-tetramethylpiperidine-N-oxyl (TEMPONE). Eur J Pharm Sci.
11 Li H., He G., Deng Y., Kuppusamy P., Zweier J.L. (2006). In vivo proton electron double resonance imaging of the distribution and clearance of nitroxide radicals in mice. Magn Reson Med.
12 Hyodo F., Yasukawa K., Yamada K., Utsumi H. (2006). Spatially resolved time-course studies of free radical reactions with an EPRI/MRI fusion technique. Magn Reson Med.
13 Sosnovsky G., Konieczny M. (1976). Preparation of triacetoneamine (4-oxo-2,2,6,6-tetramethylpiperidine), an improved method. Synthesis.
14 Zhdanov, R.I., Nitroxyl radicals and non-radical reactions of free radicals. Bioactive spin labels, ed. R.I. Zhdanov. 1992, New York: Springer-verlag. 26.
15 Sano H., Matsumoto K., Utsumi H. (1997). Synthesis and imaging of blood-brain-barrier permeable nitroxyl-probes for free radical reactions in brain of living mice. Biochem Mol Biol Int.
16 Okajo A., Matsumoto K., Mitchell J.B., Krishna M.C., Endo K. (2006). Competition of nitroxyl contrast agents as an in vivo tissue redox probe: comparison of pharmacokinetics by the bile flow monitoring (BFM) and blood circulating monitoring (BCM) methods using X-band EPR and simulation of decay profiles. Magn Reson Med.